# ^99m^Tc- anti-EGFR monoclonal antibody h-R3

Chemical name: | ^99m^Tc-labeled humanized anti-EGFR monoclonal antibody h-R3
Abbreviated name: | ^99m^Tc-hR3
Synonym: | DiaCIM
Agent Category: | anti-EGFR monoclonal antibody h-R3
Target: | Epidermal growth factor receptor
Target Category: | Binding
Method of detection: | SPECT
Source of signal: | ^99m^Tc
Activation: | Not required
Studies: | - In vitro; - Rodents; - Humans | View human EGFR protein and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_005228) sequences.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20anti%20egfr%20monoclonal%20antibody%20hr3)]

Overexpression of the epidermal growth factor receptor (EGFR) is a characteristic feature of a variety of cancers such as squamous cell lung carcinoma and breast, ovarian, head and neck, bladder, and colon cancers (1). The EGFR is a 170-kDa transmembrane protein that promotes cell proliferation by the specific binding of the autocrine epidermal growth factor (EGF) and transforming growth factor α (TGFα). The activity of these factors is believed to contribute to the progression of cancers. This EGFR operates through a receptor-associated tyrosine kinase–mediated signal transduction pathway. In an effort to develop therapy against cancer, a variety of EGFR inhibitors have been developed that either inhibit activation of the receptor kinase or inhibit the binding of EGF and TGFα, e. g., monoclonal antibodies (MAb) to the receptor (2).

A murine MAb ior egf/r3, with a high affinity for an extracellular domain of the EGFR, was developed and tested for the treatment of cancers (3). This MAb was also labeled with radioactive technetium (^99m^Tc) for molecular imaging of the EGFR in tumors to possibly predict responses to a variety of therapeutic agents under development for the treatment of cancers (4). However, because of its immunogenicity, the ^99m^Tc-labeled ior egf/r3 MAb had limited clinical utility, particularly if repeated imaging investigations were necessary (3). To circumvent this problem, a humanized form of ior egf/r3 was developed by combining the complimentary determining regions of the murine antibody with a human IgG_1_ framework (5). This humanized antibody had a low affinity for the receptor, but with modification of the structure hR3, an antibody with a similar receptor affinity as the original murine MAb, was obtained.

The hR3 was subsequently labeled with ^99m^Tc and investigated for its tissue distribution and imaging properties (3, 6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20anti%20egfr%20monoclonal%20antibody%20hr3%20synthesis)]

To produce the humanized MAb h-R3, a murine IgG_2a_ antibody ior egf/r3 secreting hybridoma was initially obtained by the fusion of murine myeloma SP2/Ag14 cells with splenocytes from Balb/c mice immunized with a partially purified human placental tissue EGFR as described elsewhere (7). The variable regions of the ior egf/e3 were cloned and a reshaped antibody was constructed using the heavy and light chains of REI and Eu, respectively, as the human immunoglobulin framework to graft the complimentary determining regions (5). The antibodies were reduced with mercaptoethanol in phosphate-buffered saline at room temperature for 30 min and purified on a Sephadex G-50 gel filtration column.

Aliquots of the reduced mAb (3 mg each) formulated in 15 mg glucose were dispensed in 10-ml vials and instantly frozen with liquid nitrogen (8). To each vial 150 µl of the methyl diphosphonate (MDP) bone scanning kit (dissolved in normal saline) was added to obtain 50 µg MDP, 3.4 µg stannous acid, and 20 µg p-aminobenzoic acid per mg MAb. The vials were once again frozen with liquid nitrogen, lyophilized for 24 h, sealed under vacuum, and stored as a kit at 4ºC until required (8).

To radiolabel the agent, the lyophilized MAb was reconstituted with 1–2 ml (30 mCi) pertechnetate (TcO_4_^-^) and the contents were dissolved by gently swirling the vial. To complete the labeling reaction, the vial was left at room temperature for 10 min. The average number of –SH groups per molecule, as measured by a cysteine assay, was 5.28 ± 0.06, and the specific activity of the labeled MAb, as determined by paper chromatography, was 10 mCi/58.8 nmol protein with a labeling efficiency of 99.21 ± 0.42% (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20anti-EGF-r%20monoclonal%20antibody%20h-R3%20in%20vitro)]

The immunorectivity of ^99m^Tc-hR3 was compared to the murine ior egf/r3 antibody by use of a radioreceptor assay (8). The humanized MAbs were determined to have an inhibition constant (K_i_) that was similar to the original mouse antibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20hR3%20rodentia)]

The biodistribution of ^99m^Tc-hR3 was determined in nude mice bearing A431 human epidermoid carcinoma cell tumors (8). The mice were sacrificed 4 and 24 h after administration of ^99m^Tc-hR3. Radioactivity levels in the tumors, heart, liver, kidney, lungs, stomach, spleen, and intestines were determined. In general, accumulation of radioactivity was evident in the serum, the kidneys, and the spleen. A significant accumulation of radioactivity as compared to the other organs was observed in the kidneys and the spleen both at 4 and 24 h post injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20hR3%20non-primate%20mammals)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20anti-EGF-r%20monoclonal%20antibody%20h-R3%20Non-Human%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-%20anti-EGF-r%20monoclonal%20antibody%20h-R3%20Humans)]

The safety, localization in normal tissue and tumor, pharmacokinetics, and radiation dosimetry of ^99m^Tc-hR3 in patients with recurrent or metastatic epithelial malignancies were evaluated (3). Either 3.0 mg/505 MBq (3.0 mg/13.64 mCi) or 6.0 mg/1,010 MBq (6.0 mg/27.29 mCi) ^99m^Tc-hR3 was administered to the patients. Whole-body imaging was performed up to 24 h after administration and the normal organ uptake was quantified. Patients showed no adverse effects and no changes in biochemical/hematological indices or immune response to ^99m^Tc-hR3. Tissue uptake was found mainly in the liver, spleen, and the kidneys. One patient was found by use of single-photon emission computed tomography (SPECT) analysis to be positive for squamous cell carcinoma of the mouth involving the lymph nodes. It was concluded ^99m^Tc-hR3 had an excellent safety profile and that a larger group of patients pre-selected for EGFR positivity should be included in a clinical trial for further study.

In another clinical trial, the biodistribution, organ radiation dosimetry, and toxicity of ^99m^Tc-hR3 were investigated in humans (6). Patients with suspected epithelium-derived tumors were divided into two groups: patients in group 1 received a dose of 3 mg/1,110 MBq (3 mg/30 mCi) of ^99m^Tc-hR3, and patients in group 2 received a dose of 6 mg/2,220 MBq (6 mg/60 mCi) of the labeled antibody. Biodistribution of the antibody was monitored by use of SPECT, and multiple samples of blood and urine were collected for up to 24 h. The liver, spleen, kidneys, bladder, and heart were identified as the main organs for accumulation of radioactivity in these patients. The liver had the highest absorbed dose, followed by the kidneys and the urinary bladder wall with an excretion of ~22% of the injected dose in the urine. A preliminary analysis of the results suggested that the labeled antibody had a sensitivity of 76.5% and a specificity of 100%. It was concluded that ^99m^Tc-hR3 was safe for use in humans and could be used for diagnosis of epithelium-derived tumors at the two doses used in the study.

## References

1 Gullick W.J. (1991). Prevalence of aberrant expression of the epidermal growth factor receptor in human cancers. Br Med Bull.
2 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
3 Vallis K.A., Reilly R.M., Chen P., Oza A., Hendler A., Cameron R., Hershkop M., Iznaga-Escobar N., Ramos-Suzarte M., Keane P. (2002). A phase I study of 99mTc-hR3 (DiaCIM), a humanized immunoconjugate directed towards the epidermal growth factor receptor. Nucl Med Commun.
4 Ramos-Suzarte M., Rodriguez N., Oliva J.P., Iznaga-Escobar N., Perera A., Morales A., Gonzalez N., Cordero M., Torres L., Pimentel G., Borron M., Gonzalez J., Torres O., Rodriguez T., Perez R. (1999). 99mTc-labeled antihuman epidermal growth factor receptor antibody in patients with tumors of epithelial origin: Part III. Clinical trials safety and diagnostic efficacy. J Nucl Med.
5 Mateo C., Moreno E., Amour K., Lombardero J., Harris W., Perez R. (1997). Humanization of a mouse monoclonal antibody that blocks the epidermal growth factor receptor: recovery of antagonistic activity. Immunotechnology.
6 Torres L.A., Perera A., Batista J.F., Hernandez A., Crombet T., Ramos M., Neninger E., Perez M., Sanchez E.L., Romero S., Aguilar V., Coca M.A., Iznaga-Escobar N. (2005). Phase I/II clinical trial of the humanized anti-EGF-r monoclonal antibody h-R3 labelled with 99mTc in patients with tumour of epithelial origin. Nucl Med Commun.
7 Fernandez A., Spitzer E., Perez R., Boehmer F.D., Eckert K., Zschiesche W., Grosse R. (1992). A new monoclonal antibody for detection of EGF-receptors in western blots and paraffin-embedded tissue sections. J Cell Biochem.
8 Morales A.A., Duconge J., Alvarez-Ruiz D., Becquer-Viart M.L., Nunez-Gandolff G., Fernandez E., Caballero-Torres I., Iznaga-Escobar N. (2000). Humanized versus murine anti-human epidermal growth factor receptor monoclonal antibodies for immunoscintigraphic studies. Nucl Med Biol.